# Alexa Fluor 680-Bevacizumab

Chemical name: | Alexa Fluor 680-Bevacizumab
Abbreviated name: | Alexa680-Bevacizumab
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor (VEGF)
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence
Source of signal/contrast: | Alexa Fluor 680 (Alexa680)
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350–700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (3). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species do (4). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (3).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (5). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (6, 7). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (8-10). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease (11, 12). Therefore, it is important to measure VEGF levels in the tumors to design better anti-cancer treatment protocols. Bevacizumab is a humanized antibody against VEGF-A. It binds to all VEGF isoforms. Bevacizumab is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer. Chang et al. (13) prepared Alexa Fluor 680-bevacizumab (Alexa680-bevacizumab) for imaging VEGF expression in tumors. Alexa680 is a NIR fluorescent dye with absorbance maximum at 684 nm and emission maximum at 707 nm with a high extinction coefficient of 183,000 (mol/L)^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+synthesis)]

Alexa Fluor 680 N-succinimidyl ester and bevacizumab were incubated in sodium bicarbonate buffer (pH 9) for 60 min at room temperature (13). Alexa680-bevacizumab was isolated from the incubation mixture with column chromatography. There were six dye molecules per antibody molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+rodentia)]

Chang et al. (13) performed biodistribution studies of Alexa680-bevacizumab in mice bearing PC-3 prostate, AsPC-1 pancreatic, or Capan-1 pancreatic tumors. Images were obtained after injection of 100 μg Alexa680-bevacizumab at 1, 3, 6, and 24 h. Substantial contrasts were observed between the tumors and normal tissue as early as 1 h. Fluorescent intensity increased during the first 6 h and leveled by 24 h. Negligible fluorescence uptake into the tumors was observed with injection of Alexa680 or Alexa680-IgG. There was a linear correlation between the level of Alexa680-bevacizumab accumulation and the level of VEGF expression in the tumor homogenates as determined with ELISA. There was also a good correlation between the level of Alexa680-bevacizumab accumulation and the tumor microvessel density, as measured with histoimmunochemistry (r = 0.64, P < 0.05). Pretreatment with bevacizumab (1 mg/mouse) in mice bearing PC-3 tumors (3.4 contrast units) reduced fluorescent uptake into the tumor (2.0 contrast units), whereas BSA (1 mg/mouse) and MLN591 antibody (1 mg/mouse) showed no reduction. Photodynamic therapy delivered to the tumor-bearing mice showed a two-fold increase in both tumor Alexa680-bevacizumab accumulation and VEGF concentration as shown previously (11, 12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+human)]

No publication is currently available.

## NIH Support

P01 CA84203

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
4 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
5 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
6 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
7 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
8 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
9 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
10 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
11 Gorski D.H., Beckett M.A., Jaskowiak N.T., Calvin D.P., Mauceri H.J., Salloum R.M., Seetharam S., Koons A., Hari D.M., Kufe D.W., Weichselbaum R.R. (1999). Blockage of the vascular endothelial growth factor stress response increases the antitumor effects of ionizing radiation. Cancer Res.
12 Solban N., Selbo P.K., Sinha A.K., Chang S.K., Hasan T. (2006). Mechanistic investigation and implications of photodynamic therapy induction of vascular endothelial growth factor in prostate cancer. Cancer Res.
13 Chang S.K., Rizvi I., Solban N., Hasan T. (2008). In vivo optical molecular imaging of vascular endothelial growth factor for monitoring cancer treatment. Clin Cancer Res.